# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-E{E[c(RGDyK)]_2_}_2_

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid- E{E[c(RGDyK)]_2_}_2_
Abbreviated name: | ^64^Cu-DOTA-E{E[c(RGDyK)]_2_}_2_, ^64^Cu-tetrameric RGD D-Tyr analog
Synonym: | ^64^Cu-Tetrameric RGD peptide
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov). Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(RGD+tetramer)+OR+(64Cu-DOTA-RGD+tetramer))]

^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-E{E[c(RGDyK)]_2_}_2_ (^64^Cu-DOTA-E{E[c(RGDyK)]_2_}_2_) is an integrin-targeted molecular imaging agent developed for positron emission tomography (PET) imaging of tumor vasculature, tumor angiogenesis, and osteoclasts (1). ^64^Cu is a positron emitter with a half-life (t_½_) of 12.7 h.

Cellular survival, invasion, and migration control embryonic development, angiogenesis, tumor metastasis, and other physiological processes (2, 3). Among the molecules that regulate angiogenesis are integrins, which comprise a superfamily of cell-adhesion proteins that form heterodimeric receptors for extracellular matrix (ECM) molecules (4, 5). These transmembrane glycoproteins consist of two noncovalently associated subunits, α and β (18 α- and 8 β-subunits in mammals), which are assembled into at least 24 α/β pairs. Several integrins, such as integrin α_v_β_3_, have affinity for the arginine-glycine-aspartic acid (RGD) tripeptide motif, which is found in many ECM proteins. Expression of integrin α_v_β_3_ receptors on endothelial cells is stimulated by angiogenic factors and the environment. The integrin α_v_β_3_ receptor is generally not found in normal tissue but it is strongly expressed in vessels with increased angiogenesis, such as tumor vasculature. It is significantly upregulated in certain types of tumor cells and in almost all tumor vasculature. Molecular imaging probes carrying the RGD motif that binds to the integrin α_v_β_3_ can be used to image tumor vasculature and evaluate angiogenic response to tumor therapy (6, 7).

Various RGD peptides in both linear and cyclic forms have been developed for in vivo binding to integrin α_v_β_3_ (8). It has been hypothesized that cyclic RGD peptides (RGDfK or RGDyK) may have a faster rate of receptor binding or a slower rate of dissociation from the integrin α_v_β_3_ than linear single-RGD peptides (9). Chen et al (10). evaluated a cyclic RGD D-Tyr analog peptide [c(RGDyK)] labeled with ^64^Cu or ^18^F in nude mice bearing breast tumors. They used DOTA for c(RGDyK) conjugation with ^64^Cu; ^64^Cu-DOTA-c(RGDyK) showed prolonged tumor radioactivity retention but persistent liver radioactivity. Wu et al. (9) suggested that a multimeric RGD peptide with more than two repeating cyclic RGD units would further enhance the affinity of the receptor−ligand interactions through a polyvalency effect. They also suggested that the increase in molecular size might prolong circulation time and reduce tumor washout rate as well. Consequently, Wu et al. (9) developed the tetrameric RGD D-Phe analog peptide ^64^Cu-DOTA-E{E[c(RGDfK)]_2_}_2_ and showed that this PET radioligand appeared to have high integrin avidity and favorable biokinetics in nude mice bearing human gliomas. Li et al. (1) also prepared the tetrameric ^64^Cu-DOTA-E{E[c(RGDyK)]_2_}_2_ and octameric ^64^Cu-DOTA-E(E{E[c(RGDyK)]_2_}_2_)_2_ for evaluation.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(RGD+tetramer)+OR+(64Cu-DOTA-RGD+tetramer))]

Li et al. (1) reported the synthesis of the tetrameric ^64^Cu-DOTA-E{E[c(RGDyK)]_2_}_2_. DOTA-E{E[c(RGDyK)]_2_}_2_ was synthesized through an active ester method by coupling Boc-Glu(OSu)-OSu with E[c(RGDyK)]_2_ followed by deprotection. The monomeric cyclic peptide c(RGDyK) was first prepared via solution cyclization of fully protected linear pentapeptide H-Gly-Asp(OtBu)-D-Tyr(OtBu)-Lys(Boc)-Arg(Pbf)-OH, followed by trifluoroacetic acid (TFA) deprotection in the presence of the free-radical scavenger triisopropylsilane (9, 11). The RGD dimer was then prepared by mixing c(RGDyK) with the Boc-protected, glutamic acid–activated ester Boc-Glu(OSu)_2_ in triethylamine and stirring at room temperature overnight (11, 12). This yielded Boc-E[c(RGDyK)]_2._ The Boc-group was then removed using anhydrous TFA. Similarly, the tetramer was prepared by mixing E[c(RGDyK)]_2_ with Boc-E(OSu)_2_ at room temperature (pH 8.5−9.0) overnight and removing the Boc-group by treatment with TFA. E{E[c(RGDyK)]_2_}_2_ was purified with high-performance liquid chromatography (HPLC) (9). DOTA-E{E[c(RGDyK)]_2_}_2_ was synthesized by first activating DOTA with 1-ethyl-3-[3-(dimethylamino)propyl]carbodiimide and N-hydroxysulfonosuccinimide (pH 5.5) for 30 min to produce DOTA-OSSu. DOTA-OSSu was then cooled to 4ºC and reacted with E{E[c(RGDyK)]_2_}_2_. The reaction mixture was adjusted to pH 8.5 and incubated overnight. The DOTA-peptide was purified with semi-preparative HPLC with a yield of 70%. Matrix-assisted laser desorption/ionization time-of-flight mass spectrometry showed a molecular weight of 3,199.0, which was in agreement with the calculated value of 3,198.4 (C_140_H_207_N_42_O_45_). ^64^Cu-DOTA-E{E[c(RGDyK)]_2_}_2_ was prepared by adding 37 MBq ^64^Cu-chloride/5 μg peptide (1 mCi/5 μg peptide) in sodium acetate to DOTA-E{E[c(RGDyK)]_2_}_2_ and incubating for 1 h at 50ºC. The final radiolabeled peptide was purified by semi-preparative HPLC. The radiochemical yield was 80–90% (decay-corrected). The radiochemical purity was >98%, and the specific activity was 23 MBq/nmol (0.62 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((RGD+tetramer)+OR+(64Cu-DOTA-RGD+tetramer))+AND+in+vitro)]

Li et al. (1) conducted an in vitro cell integrin receptor-binding assay of unlabeled DOTA-E{E[c(RGDyK)]_2_}_2_, using ^125^I-echistatin as the integrin-specific radioligand and integrin α_v_β_3_−positive human glioblastoma U87MG cells. The cell-binding assay demonstrated that DOTA had minimal effect on the receptor avidity. The 50% inhibitory concentration (IC_50_) value for DOTA-E{E[c(RGDyK)]_2_}_2_ was (2.8 ± 0.4) × 10−^8^ M (n = 3). In comparison, the IC_50_ value for E{E[c(RGDyK)]_2_}_2_ was (3.5 ± 0.3) × 10−^8^ M. This tetramer also had ~three-fold higher affinity than the dimeric E[c(RGDyK)]_2._ In vitro cell adhesion assays were also conducted to investigate the effect of E{E[c(RGDyK)]_2_}_2_ on U87MG cell adhesion (1). E{E[c(RGDyK)]_2_}_2_ had no effect on the cell adhesion ability in the presence of fibronectin, but the tetramer inhibited cell adhesion in a concentration-dependent manner in the presence of vitronectin. The calculated IC_50_ value was (3.2 ± 0.9) × 10−^7^ M (n = 4). In comparison, the IC_50_ value for the dimeric E[c(RGDyK)]_2_ was (7.0 ± 1.0) × 10−^7^ M.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(RGD+tetramer)+OR+(64Cu-DOTA-RGD+tetramer))]

Biodistribution studies of ^64^Cu-DOTA-E{E[c(RGDyK)]_2_}_2_ were conducted in normal nude mice (n = 3) (1). Each mouse received an i.v. dose of 0.74−1.11 MBq (20−30 μCi) ^64^Cu-DOTA-E{E[c(RGyK)]_2_}_2_ and was then euthanized 20 h after injection. The tumor radioactivity level in the kidney was 5.0 ± 0.7% injected dose per gram (% ID/g). The liver radioactivity level was ~2% ID/g (extrapolated from Figure 5A). The blood radioactivity level was ~0.1% ID/g, and the muscle radioactivity level was ~0.2% ID/g. Coinjection dose of 10 mg/kg c(RGDyK) significantly decreased the radioactivity in all tissues. The radioactivity level of the kidney was decreased to ~2.0% ID/g (extrapolated from Figure 5B). The liver radioactivity level was reduced to ~0.5% ID/g.

MicroPET imaging was conducted in nude mice bearing s.c. U87MG tumors (100–400 mm^3^) and c-neu oncomice (integrin α_v_β_3_-positive) that developed spontaneous mammary adenocarcinomas (1). Each mouse was injected with an i.v. dose of 9.3 MBq (0.25 mCi). ^64^Cu-DOTA-E{E[c(RGDyK)]_2_}_2_ clearly visualized the tumor with high tumor/background contrast up to 20 h after injection. Quantitative analyses of PET imaging data showed that the radioactivity levels in the U87MG tumors (n = 3) were 10.3 ± 1.6% ID/g (0.5 h), 9.6 ± 1.4% ID/g (1 h), 8.6 ± 1.0% ID/g (2 h), 7.7 ± 1.6% ID/g (6 h), and 6.4 ± 0.7% ID/g (20 h). The liver radioactivity level was ~3% ID/g at 0.5 h and then decreased to ~2% ID/g at 20 h (extrapolated from Figure 4A). The kidney radioactivity level decreased from ~10% ID/g at 0.5 h to ~5% ID/g at 20 h, and the muscle radioactivity level decreased from ~1.5% ID/g at 0.5 h to ~0.5% ID/g at 20 h. In comparison, the tumor radioactivity appeared to be slightly higher than that of the D-Phe tetrameric analog ^64^Cu-DOTA-E{E[c(RGDfK)]_2_}_2_. The liver and kidney radioactivity levels of the D-Tyr and D-Phe analogs were similar. Coinjection with a dose of 10 mg/kg c(RGDyK) significantly decreased the radioactivity levels in the tumor, liver, kidney, and muscle at 2 h after injection. The tumor radioactivity level was reduced from ~8.8% ID/g to ~2.2% ID/g at 2 h after injection (extrapolated from Figure 5C). The kidney radioactivity level was reduced from ~5% ID/g to ~1.9% ID/g at 2 h after injection. In the c-neu oncomouse model of spontaneous mammary tumors, the tumor radioactivity levels were 4.4 ± 0.9% ID/g at 1 h and 3.6 ± 0.4% ID/g at 20 h. The liver and kidney radioactivity levels between 1 and 20 h after injection were ~2.5% ID/g and ~5% ID/g, respectively (extrapolated from Figure 4B). The muscle radioactivity level decreased from ~0.83% ID/g at 1 h to ~0.46% ID/g at 20 h.

Wu et al. (9) estimated the radiation-absorbed doses of ^64^Cu-DOTA-E{E[c(RGDfK)]_2_}_2_ in the adult human on the basis of the average biodistribution data in nude mice bearing U87MG tumors. The urinary bladder wall appeared to be the critical organ with 0.262 ± 0.0472 mGy/MBq (0.969 ± 0.175 rad/mCi). The total body dose was 0.00235 ± 0.000376 mGy/MBq (0.00869 ± 0.00139 rad/mCi). The estimated doses to the kidneys and liver were 0.0296 ± 0.00184 mGy/MBq (0.110 ± 0.00684 rad/mCi) and 0.0243 ± 0.00156 mGy/MBq (0.0898 ± 0.00576 rad/mCi), respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((RGD+tetramer)+OR+(64Cu-DOTA-RGD+tetramer))+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((RGD+tetramer)+OR+(64Cu-DOTA-RGD+tetramer))+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((RGD+tetramer)+OR+(64Cu-DOTA-RGD+tetramer))+AND+human)]

## References

1 Li Z.B., Cai W., Cao Q., Chen K., Wu Z., He L., Chen X. (2007). (64)Cu-labeled tetrameric and octameric RGD peptides for small-animal PET of tumor alpha(v)beta(3) integrin expression. J Nucl Med.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Paulhe F., Manenti S., Ysebaert L., Betous R., Sultan P., Racaud-Sultan C. (2005). Integrin function and signaling as pharmacological targets in cardiovascular diseases and in cancer. Curr Pharm Des.
4 Hood J.D., Cheresh D.A. (2002). Role of integrins in cell invasion and migration. Nat Rev Cancer.
5 Hwang R., Varner J. (2004). The role of integrins in tumor angiogenesis. Hematol Oncol Clin North Am.
6 Cai W., Shin D.W., Chen K., Gheysens O., Cao Q., Wang S.X., Gambhir S.S., Chen X. (2006). Peptide-labeled near-infrared quantum dots for imaging tumor vasculature in living subjects. Nano Lett.
7 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
8 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
9 Wu Y., Zhang X., Xiong Z., Cheng Z., Fisher D.R., Liu S., Gambhir S.S., Chen X. (2005). microPET imaging of glioma integrin {alpha}v{beta}3 expression using (64)Cu-labeled tetrameric RGD peptide. J Nucl Med.
10 Chen X., Park R., Tohme M., Shahinian A.H., Bading J.R., Conti P.S. (2004). MicroPET and autoradiographic imaging of breast cancer alpha v-integrin expression using 18F- and 64Cu-labeled RGD peptide. Bioconjug Chem.
11 Chen X., Park R., Shahinian A.H., Bading J.R., Conti P.S. (2004). Pharmacokinetics and tumor retention of 125I-labeled RGD peptide are improved by PEGylation. Nucl Med Biol.
12 Liu S., Hsieh W.Y., Kim Y.S., Mohammed S.I. (2005). Effect of coligands on biodistribution characteristics of ternary ligand 99mTc complexes of a HYNIC-conjugated cyclic RGDfK dimer. Bioconjug Chem.
.